# [^99m^Tc]-diethylenetriaminepentaacetic acid-galactosyl human serum albumin

Chemical name: | [^99m^Tc]-diethylenetriaminepentaacetic acid-galactosyl human serum albumin | [image]
Abbreviated name: | ^99m^Tc-GSA | [image]
Synonym: | Technetium-[^99m^Tc]-galactosyl human serum albumin, ^99m^Tc-galactosyl-neoglycoalbumin, ^99m^Tc-DTPA-GSA, ^99m^Tc-NGA | [image]
Agent Category: | Protein | [image]
Target: | Asialoglycoprotein | [image]
Target Category: | Receptors | [image]
Method of detection: | Single photon emission computed tomography (SPECT); planar gamma imaging | [image]
Source of signal / contrast: | ^99m^Tc | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents; - Non-human primates; - Humans | The structure of ^99m^Tc-GSA. N = number of galactose molecules bound to HSA. M = number of DTPA molecules. The exact coordinates of ^99m^Tc are unknown.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc-GSA)]

The primary function of the liver is to remove toxins from the body through metabolism and excretion, and to synthesize complex biologically active substances such as clotting factors and albumin. Impairment of liver function as a result of hepatitis, infections, jaundice, cirrhosis, or cancer can lead to a variety of gastrointestinal disorders. The evaluation of hepatic function is an important parameter in the determination of the physiological state of the liver, particularly for patients who have been diagnosed with liver disease for which a hepatectomy or liver transplantation is the treatment of choice (1). Therefore, determination of the hepatic function is now considered important before and after a hepatectomy or liver transplantation to predict patient outcome (2).

The asialoglycoprotein receptors (ASGP-R) exist specifically on hepatic cell membranes and are believed to be necessary for intracellular trafficking and endocytic activity in the liver. The number of ASGP-R on the hepatocytes of individuals with liver disease is altered and is thus considered a good indicator for the evaluation of liver function (3, 4). Technetium [^99m^Tc]-diethylenetriaminepentaacetic acid-galactosyl-human serum albumin (^99m^Tc-GSA), originally known as ^99m^Tc-galactosyl-neoglycoalbumin (^99m^Tc-NGA), is an ASGP-R ligand that accumulates specifically in the liver and is used for liver scintigraphy to determine hepatocyte mass and function (1, 5, 6). ^99m^Tc-GSA is available as a commercial kit in Japan (www.nmp.co.jp/eng/about/index.html, in English, and www.nmp.co.jp/index.html, in Japanese). According to Stadalnik and Vera, ^99m^Tc-GSA has been available only at one institution in the United States, the University of California, Davis Medical Center (6).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc-GSA%20synthesis)]

The synthesis of ^99m^Tc-GSA in the laboratory was described by Kudo et al. (7). Galactose was derivatized to produce cyanomethyl 2,3,4,6-tetra-O-acetyl-1-thio-β-D-galactose (CNM-thiogalactose). The CNM-thiogalactose was purified by repeated recrystallization from dry methanol. It was then re-dissolved in methanol, and sodium methoxide was added to the solution. This mixture was kept at room temperature for 48 h. The solvent was evaporated in vacuo at 40^o^C to obtain 2-imino-2-methoxyethyl-1-thio- β-D-galactose (IME-thiogalactose). This reaction step had an estimated yield of 55%.

Human serum albumin (HSA), diluted in borate buffer at pH 8.5, was added to IME-thiogalactose, and the mixture was stirred at 37^o^C for 1.5 h to yield HSA derivatives with 30–40 moles of galactose coupled per mole of HSA. Subsequently, cyclic diethylenetriaminepentaacetic acid (cDTPA) was slowly added to the reaction mixture, and the coupling was allowed to proceed for 10 min at 37^o^C with continuous stirring. This reaction yielded HSA derivatives containing 4.5–7.0 moles of DTPA per mole of HSA. The GSA monomers were isolated from the HSA derivative mixture by high-performance liquid chromatography (HPLC) using a NaCl solution as the elution solvent. GSA obtained by this method was >95% pure. The amount of galactose bound to HSA and the degree of DTPA conjugation was determined by methods described by Kudo et al. (7).

To radiolabel GSA with metastable ^99m^Tc, the concentration of HPLC-purified GSA was adjusted to 3 mg/ml at pH 3.1–3.4. The solution was deoxygenated by flushing argon gas through it until the oxygen concentration became <100 parts per billion. Then SnCl_2_ and ascorbic acid were added to obtain a final concentration of 0.1 and 0.5 µM, respectively. The solution was then dispensed into glass vials (each with a rubber stopper) through a 0.22-µm filter membrane. At this stage the vials may be frozen for the short term or lyophilized for long-term storage. To obtain ^99m^Tc-GSA, a ^99m^Tc solution was added to each vial and mixed gently at room temperature for ~1 min. Purity of ^99m^Tc-GSA was determined to be >98% by thin-layer chromatography. Specific activity of the final product obtained with this method was not provided by the authors.

Another procedure, described by Vera et al., is also available for the preparation of ^99m^Tc-NGA (8).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc-GSA%20in%20vitro)]

Using patient biopsies, Kudo et al. (9, 10) concluded that hepatic uptake of ^99m^Tc-NGA could be used to quantify ASGP-R in the liver.

In an effort to understand the occurrence of hepatic ischemia/reperfusion injury under clinical conditions, ^99m^Tc-GSA was used to characterize ASGP-R in primary cultured rat hepatocytes under hypoxic conditions (5). The maximal binding (B_max_) of ^99m^Tc-GSA to the hepatocyte membranes and ketone body ratio (KBR) that reflects cell injury in the medium was determined for three durations of hypoxia (1, 2, and 3 h). The B_max_ for receptor binding and endocytosis decreased (ng/dish) with the increase in hypoxia, although the number of viable cells remained constant. The KBR was also significantly decreased during hypoxic conditions, which indicated that the extent of cell injury depended on duration of hypoxia. The investigators concluded that the hypoxic conditions reduced the number of ASGP-R binding sites involved in endocytosis per hepatocyte and that the cells were irreversibly injured if maintained under these conditions for a prolonged period.

In another study that used cultured primary hepatocytes, Hata and Ishii showed that galactose inhibited the binding to and the internalization of ^99m^Tc-GSA into the hepatocytes (11).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc-GSA%20rodentia)]

Toxicological studies with ^99m^Tc-NGA were performed in mice and rabbits (8), and the animals showed no toxicological effects with the treatment. In a biodistribution study of rabbits, the investigators demonstrated that ^99m^Tc-NGA accumulated primarily in the liver of these animals, and almost no radioactivity was accumulated in the other organs.

The biodistribution of ^99m^Tc-GSA has been reported for rats and rabbits (7). Ten minutes after injection of ^99m^Tc-GSA, 92.4% of the injected radioactivity was found in the liver, and 74.8% of the injected dose was excreted through the hepatobiliary route into the feces at 48 h. The investigators performed ^99m^Tc-GSA imaging studies in rabbits and reported no accumulation of radioactivity in the spleen or bone marrow of the animals.

The use of ^99m^Tc-GSA scintigraphy for intraperitoneal (i.p.) imaging of tumors in a nude mouse model was investigated (12). The nude mice were inoculated with either human SHIN-3 (ovarian cancer) or LS 180 (colon cancer) cells to establish the tumors. Radiolabeled GSA was injected into the tumor-bearing mice and the biodistribution of radioactivity was examined. The tumors were clearly visible by scintigraphic imaging and the investigators concluded that ^99m^Tc-GSA imaging was useful for the imaging of i.p. tumors.

^99m^Tc-GSA scintigraphy was suggested to be useful in evaluating hepatic tissue blood flow (13, 14) and fatty liver and ischemia-reperfusion injury (15) in rats.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc-GSA%20Non-Primate%20Mammals)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc-GSA%20Non-Human%20Primates)]

The biodistribution of ^99m^Tc-NGA was studied in baboons (8) and the investigators showed that 80–90% of the injected radioactivity accumulated in the liver of these animals within 12 to 15 min after the injection.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc-GSA%20Humans)

Virgolini et al. demonstrated that ^99m^Tc-NGA scintigraphy could be used to detect liver disease, including cirrhosis and viral hepatitis, by quantification of the ASGP-R (16). In another study it was shown that ^99m^Tc-NGA scintigraphy could be used for the differential diagnosis of hepatic focal nodular hyperplasia and hepatic tumors (17).

Using ^99m^Tc-GSA for scintigraphy of the liver, Le et al. (18) devised a method to obtain a quantitative index to analyze the regional ASGP-R concentration to assess regional function of the liver. Similarly, Onodera et al. (19) used ^99m^Tc-GSA clearance from the blood pool and its binding to the ASGP-R to devise a liver uptake ratio to assess liver functional reserve. ^99m^Tc-GSA scintigraphy was also used to detect changes in functional volume of individual lobes of the liver and was suggested to be a better method than computed tomography for the detection of morphological changes in the organ (20). Hirai et al. (21) suggested that ^99m^Tc-GSA scintigraphy was a useful technique to evaluate preoperative portal embolism and postoperative liver failure after a hepatectomy.

^99m^Tc-GSA scintigraphy has also been used in humans to establish the prognosis of patients with hepatic cirrhosis (22), predict the clinical outcome of hepatitis C after interferon treatment (23), and to evaluate hepatic regional reserve changes before and after chemolipiodolization in hepatocellular carcinoma patients (24).

## Supplemental Information

[Disclaimer]

No supplemental information is currently available.

## References

1 Clavien P.A., Petrowsky H., DeOliveira M.L., Graf R. (2007). Strategies for safer liver surgery and partial liver transplantation. N Engl J Med.
2 Ishikawa M., Yogita S., Miyake H., Fukuda Y., Harada M., Wada D., Tashiro S. (2002). Clarification of risk factors for hepatectomy in patients with hepatocellular carcinoma. Hepatogastroenterology.
3 Stockert R.J. (1995). The asialoglycoprotein receptor: relationships between structure, function, and expression. Physiol Rev.
4 Sawamura T., Nakada H., Hazama H., Shiozaki Y., Sameshima Y., Tashiro Y. (1984). Hyperasialoglycoproteinemia in patients with chronic liver diseases and/or liver cell carcinoma. Asialoglycoprotein receptor in cirrhosis and liver cell carcinoma. Gastroenterology.
5 Kwon A.H., Inoue T., Ha-Kawa S.K. (2005). Characterization of the asialoglycoprotein receptor under hypoxic conditions in primary cultured rat hepatocytes. J Nucl Med.
6 Stadalnik R.C., Vera D.R. (2001). The evolution of (99m)Tc-NGA as a clinically useful receptor-binding radiopharmaceutical. Nucl Med Biol.
7 Kudo M., Washino K., Yamamichi Y., Ikekubo K. (1994). Synthesis and radiolabeling of galactosyl human serum albumin. Methods Enzymol.
8 Vera D.R., Stadalnik R.C., Krohn K.A. (1985). Technetium-99m galactosyl-neoglycoalbumin: preparation and preclinical studies. J Nucl Med.
9 Kudo M., Vera D.R., Trudeau W.L., Stadalnik R.C. (1991). Hepatic uptake of [99mTc]galactosyl-neoglycoalbumin is sensitive to receptor quantity. Int J Rad Appl Instrum B.
10 Kudo M., Vera D.R., Trudeau W.L., Stadalnik R.C. (1991). Validation of in vivo receptor measurements via in vitro radioassay: technetium-99m-galactosyl-neoglycoalbumin as prototype model. J Nucl Med.
11 Hata S., Ishii K. (1998). Effect of galactose on binding and endocytosis of asialoglycoprotein in cultured rat hepatocytes. Ann Nucl Med.
12 Yao Z., Zhang M., Sakahara H., Saga T., Nakamoto Y., Sato N., Zhao S., Arano Y., Konishi J. (1998). Imaging of intraperitoneal tumors with technetium-99m GSA. Ann Nucl Med.
13 Ohno K. (1997). ,.
14 Hiraguchi E. (1995). ,.
15 Kimoto M. (1996). ,.
16 Virgolini I., Muller C., Angelberger P., Hobart J., Bergmann H., Sinzinger H. (1991). Quantification of human hepatic binding protein (HBP) via 99mTc-galactosyl-neoglycoalbumin (NGA) liver scintigraphy. Wien Klin Wochenschr.
17 Kurtaran A., Muller C., Novacek G., Kaserer K., Mentes M., Raderer M., Pidlich J., Eibenberger K., Angelberger P., Virgolini I. (1997). Distinction between hepatic focal nodular hyperplasia and malignant liver lesions using technetium-99m-galactosyl-neoglycoalbumin. J Nucl Med.
18 Le T.T., Kobayashi H., Takai K., Kato K., Ishigaki T. (2003). Quantitative analysis for assessing regional function of liver by using 99mTc-GSA SPECT. Nagoya J Med Sci.
19 Onodera Y., Takahashi K., Togashi T., Sugai Y., Tamaki N., Miyasaka K. (2003). Clinical assessment of hepatic functional reserve using 99mTc DTPA galactosyl human serum albumin SPECT to prognosticate chronic hepatic diseases--validation of the use of SPECT and a new indicator. Ann Nucl Med.
20 Nanashima A., Yamaguchi H., Shibasaki S., Morino S., Ide N., Takeshita H., Tsuji T., Sawai T., Nakagoe T., Nagayasu T., Ogawa Y. (2006). Relationship between CT volumetry and functional liver volume using technetium-99m galactosyl serum albumin scintigraphy in patients undergoing preoperative portal vein embolization before major hepatectomy: a preliminary study. Dig Dis Sci.
21 Hirai I., Kimura W., Fuse A., Suto K., Urayama M. (2003). Evaluation of preoperative portal embolization for safe hepatectomy, with special reference to assessment of nonembolized lobe function with 99mTc-GSA SPECT scintigraphy. Surgery.
22 Sasaki N., Shiomi S., Iwata Y., Nishiguchi S., Kuroki T., Kawabe J., Ochi H. (1999). Clinical usefulness of scintigraphy with 99mTc-galactosyl-human serum albumin for prognosis of cirrhosis of the liver. J Nucl Med.
23 Kira T., Tomiguchi S., Takahashi M., Yoshimatsu S., Sagara K., Kurano R. (1999). Correlation of 99mTc-GSA hepatic scintigraphy with liver biopsies in patients with chronic active hepatitis type C. Radiat Med.
24 Kira T., Tomiguchi S., Takahashi M. (1998). Quantitative evaluation of the regional hepatic reserve by 99mTc-GSA dynamic SPECT before and after chemolipiodolization in patients with hepatocellular carcinoma. Ann Nucl Med.